# Gaussia princeps luciferase

Chemical name: | Gaussia princeps luciferase
Abbreviated name: | GLuc
Synonym: | Gaussia luciferase
Agent Category: | Luciferase
Target: | Non-targeted
Target Category: | Photon emission/bioluminescence
Method of detection: | Optical imaging
Source of signal: | Photons
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=12621053) sequence of G. princeps luciferase.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gluc&WebEnv=0lM4-K2PBOxVU9gbNvh9P0XD06qNBK-lGDhNhuw65hlAh9GvntmLFIcvFJOMb4y5f7ddR4tMR_UWojA%407748428072881B60_0000SID&WebEnvRq=1)]

Proteins engineered to generate fluorescent or bioluminescent signals are commonly used for the non-invasive study of a variety of biological processes and diseases in animals and humans (1-3). Usually the enhanced green fluorescent proteins, the variant red or yellow fluorescent proteins, or the bioluminescent luciferase proteins are used as reporter molecules because they produce a photo signal upon stimulation that can be tracked for the study of a dynamic biological system or phenomenon under in vitro and in vivo conditions (4-6). The luciferase family is composed of several different enzymes that catalyze light-producing, oxygen-dependent molecular reactions and have been detected across a diverse group of organisms including bacteria, fungi, insects, and marine animals (7). Among the luciferases, the firefly (Photinus pyralis) luciferase (FLuc) has been extensively studied; it requires ATP and Mg^2+^ as co-factors to function and oxidizes D-luciferin, its substrate, to release energy in the form of photons (8). The sea pansy (Renilla reniformis) is another luciferase (RLuc) that has been extensively investigated; RLuc uses coelenterazine as a substrate and does not require ATP to produce light. However, RLuc has a lower quantum yield compared with FLuc (6% versus 88%) and also shows a low enzymatic efficiency (9). With the use of commercially available molecular kits, the humanized forms of FLuc and RLuc (designated as hFLuc and hRLuc, respectively) were combined as dual reporters to image cultured cells in vivo because both enzymes used different substrates (10, 11). However, these enzymes have very specific requirements to catalyze reactions under in vivo conditions to generate sufficient signal/background ratios for imaging. Tannous et al. decided to explore the possibility of finding a superior luciferase that was more efficient and had a higher quantum yield compared with the FLuc and RLuc enzymes (12).

Gaussia princeps, a marine copepod, naturally secretes a luciferase (GLuc) that was cloned, expressed in Escherichia coli, and used as a detection agent in a DNA hybridization assay (13). Tannous et al. cloned the humanized version of the GLuc enzyme (hGLuc) into a herpes simplex virus-1 (HSV-1) amplicon under a cytomegalovirus (CMV) immediate early (IE) promoter and evaluated the bioluminescence emitted from DNA-transfected and vector-infected mammalian cells (12). The luciferase was also evaluated for imaging cultured cells in vivo after subcutaneous implantation of GLuc-transfected cells into nude mice (12). In another study, GLuc was evaluated for imaging after it was cloned into a lentivirus (LV) vector and transduced into human glioma cells that were implanted into nude mice (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gaussian+luciferase+synthesis&WebEnv=0pXJtXOc-CKsc0EhOlhpO1fw9mcnwMvGjDVJDa8ecFV4Evo9z9wQPExImQYHHE1wjhaPDXOWtyFcF60%407748428072881B60_0000SID&WebEnvRq=1)]

The cDNA encoding hGLuc, with codons optimized for mammalian cell expression, was amplified by polymerase chain reaction from a commercially available vector (http://www.nanolight.com/nanoligh.htm) with the use of appropriate primers (12). The primers introduced an EcoRI site at the 5’ end and an XhoI site at the 3’ end of the cDNA. The polymerase chain reaction product was digested with these enzymes, then gel-purified and cloned into the pHGCX amplicon plasmid described elsewhere (15) under the control of a CMV IE promoter. Because FLuc and RLuc are well studied, hFLuc or hRLuc cDNA, with codons optimized for mammalian cell expression and cloned into pHGCX as described by Shah et al., were used as controls in the study (11). All amplicon constructs were packaged in the HSV-1 virions with the use of a virus-free packaging system and a cell line derived from vero cells (http://www.atcc.org/catalog/numSearch/numResults.cfm?atccNum=CRL-1587) (15, 16). The cell growth medium containing the amplicon vector was concentrated and purified through a 25% sucrose cushion by centrifugation for 3 h at 4°C. The amplicon vector titer was determined in a serial dilution assay by fluorescent microscopy for the green fluorescent protein expressed by infected vero cells.

The hGLuc cDNA was also cloned into a LV vector under the control of a CMV promoter to produce LV-GLuc as detailed by Wurdinger et al. (14) For the same study, the hGLuc DNA was also cloned in a LV vector optimized for cyan fluorescent protein separated either by an internal ribosomal entry site or the secreted alkaline phosphatase (SEAP). Another LV construct contained the cDNA sequence for the mCherry protein separated by SEAP (the mCherry protein is described by Shaner et al. (17)). All of the respective LV constructs were produced by transfection of 293T cells (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-11268) with the LV vector plasmid pCMV∆R8.91 (the packaging genome plasmid) and the vesicular stomatitis virus envelope glycoprotein plasmid pVSV-G. The LV purification was performed by ultracentrifugation of the cell conditioned growth medium and titered as transducing units (t.u.)/ml on 293T cells in the presence of polybrene by counting the cells positive for cyan or yellow fluorescent proteins 72 h after infection (18). The typical titer was reported to be 10^8^ t.u./ml.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gaussia+luciferase+in+vitro&WebEnv=0ydff3aDKNg3owxkBrbKZ9v9vI0960FPfCTgVPM2l6tCSjXW4hDGUWAtcBfP9i2w6rxLgQ-DWMDdCrf%407748428072881B60_0000SID&WebEnvRq=1)]

Mammalian cells containing the HSV-1 amplicon vectors were reported to express the secreted hGLuc and exhibited bioluminescence characteristics that were similar to those of other coelenterazine luciferases (12). The hGLuc generated a >1,000-fold higher bioluminescent signal intensity from live cells in the presence of the growth medium and a >100-fold higher intensity from viable cells alone (in the absence of the growth medium) or cell lysates compared with either the hFLuc or the hRLuc expressed under the same conditions. Compared with hRLuc, the hGLuc had a 200-fold higher signal intensity and exhibited an intensity comparable to hFLuc under standard in vivo imaging conditions. The investigators concluded that hGLuc could provide a sensitive means to image cells and their environment in real time after gene delivery because it has a high signal intensity and is a secreted luciferase that is independent of ATP.

In another study, hGLuc was transduced into 293T cells, and its secretion was monitored by determining the conditioned medium luciferase activity (18). When the cells were treated with different drugs that interfere with the protein secretion pathway at various stages, the secretion of hGLuc was decreased up to 90%. To visualize the secretion pathway of cells in real time, the cells were co-transfected with a plasmid expressing FLuc and a plasmid expressing either hGLuc or SEAP. The FLuc activity was measured with luciferin, and it was used to normalize the hGLuc or SEAP activity. The hGLuc or SEAP activity was measured in the cell-free conditioned (growth) medium by the addition of either coelenterazine (for hGLuc) or chloro-5-substituted adamantyl-1,2-dioxetane phosphate (for SEAP). hGLuc proved very sensitive in the detection of the cellular endoplasmic reticulum (ER) stress that is associated with a temporary reduction in protein processing through the secretion pathway. The hGLuc secretion assay was reported to have a >20,000-fold higher sensitivity compared with the SEAP assay, which is a well-established technique used to monitor protein processing and ER stress in mammalian cells. The investigators concluded that the GLuc assay was a rapid, quantitative, and sensitive technique to monitor the cellular secretion pathway and ER stress that could be used for high-throughput screening to discover drugs useful in the treatment of conditions that induce or are a consequence of cellular ER stress.

Wurdinger et al implanted different amounts of human Gli36 glioma cells transduced with a LV vector encoding GLuc into the flanks of nude mice to generate tumors in the animals (14).Three days after tumor implantation, GLuc activity was measured with a luminometer by adding coelenterazine to the blood obtained from these mice. The luciferase activity in the blood was determined to be linear with respect to the number of cells implanted into the animals. Some GLuc activity was also detected in the urine of the animals, indicating that it was cleared through the kidneys. The investigators also noted that there was little difference between the activity measurements in whole blood and the serum, suggesting that hemoglobin, which normally affects luciferase activity (19), did not interfere with the GLuc activity under these assay conditions. The GLuc half-life was determined to be ~6 days when the blood or serum samples were stored at 4°C. Under in vivo conditions, the half-life of GLuc was reported to be ~20 min (14). In addition, a comparison of the GLuc and SEAP (after implantation of Gli36 cells transfected with the appropriate vectors expressing the respective enzymes into mice; see Synthesis section above for details of the vectors) activities in the blood revealed that the GLuc assay was >1,000-fold more sensitive compared with the SEAP assay because hemoglobin inhibits SEAP activity. The investigators also demonstrated that the GLuc concentration in blood could be used as a quantitative marker for the tumor cells expressing GLuc in vivo (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gaussia+luciferase+rodentia&WebEnv=0mZNCB8_x9TmOXBCNjZk0bYJ2TTnzFNLWk2_nO0WZT0rHEnTXvIuJAX2fVGv-0FQWJjRx2tiE5OeVY%407748428072881B60_0000SID&WebEnvRq=1)]

A nude mouse model (n = 4 animals/group) was used to compare the bioluminescence intensity produced by Gli36 cells respectively expressing the control (no luciferase expression), hGLuc, hFLuc, or hRLuc (12). The mice were implanted with the Gli36 cells transfected with the respective vectors, and the tumors were allowed to grow for up to 5 days. To determine the luciferase activity from the different tumors, the mice were injected with the respective substrates (25–200 μg coelenterazine/mouse for hGLuc and hRLuc, and 4 mg D-luciferine/mouse for hFLuc) through two different routes, either through the tail vein or intracardially. Under either route of administration, the bioluminescence signal obtained with GLuc was reported to be 200-fold higher than that from the tumors that expressed hRLuc and comparable to the signal obtained with the tumors that expressed FLuc as measured under identical conditions. No signal was detected in the control tumors.

To evaluate the use of hGLuc for imaging deep tissue, 1 × 10^6^ Gli36 cells expressing hGLuc were implanted in the right basal ganglia of five nude mice (12). Seven days after implantation, the bioluminescence signal from the implanted cells was detected from the tumors after an intravenous injection of 100 μg coelenterazine.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gaussia+luciferase+non+primate+mammals&WebEnv=0N-un-8OPqTJ2hH8Gt-k7OPZFcg0TYY11Xu1caczSxqxGdwSYAj-RwuX5QjLSFPkLnSidMFEigi6HAd%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gaussia+luciferase+non+human+primates&WebEnv=0ynf4GaOBSggA3pP0rPZv54jmBHkd_2khoJ4QCmI2VfvgjqSrAGZUDdLXqNYagv_T6h2vrpsgMslqYj%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gaussia+luciferase+human+studies&WebEnv=0DtCY6SMbIncU7PwX4QzMayn2ucsj6z0H8AvIhjSMEg4PToCrTY5t7AnjnUS9vqNVzVnXb_VF_9Roi_%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Parts of the studies presented in this chapter were funded by NCI grants CA69246, CA86355, CA92782, and 1K99CA126839-01.

## References

1 Barrett T., Koyama Y., Hama Y., Ravizzini G., Shin I.S., Jang B.S., Paik C.H., Urano Y., Choyke P.L., Kobayashi H. (2007). In vivo diagnosis of epidermal growth factor receptor expression using molecular imaging with a cocktail of optically labeled monoclonal antibodies. Clin Cancer Res.
2 Peterson J.R., Infanger D.W., Braga V.A., Zhang Y., Sharma R.V., Engelhardt J.F., Davisson R.L. (2008). and Longitudinal Non-invasive Monitoring of Transcription Factor Activation in Cardiovascular Regulatory Nuclei Using Bioluminescence Imaging. Physiol Genomics.
3 Zinn K.R., Chaudhuri T.R., Szafran A.A., O'Quinn D., Weaver C., Dugger K., Lamar D., Kesterson R.A., Wang X., Frank S.J. (2008). Noninvasive bioluminescence imaging in small animals. Ilar J.
4 Li Y., Sierra A.M., Ai H.W., Campbell R.E. (2008). Identification of Sites Within a Monomeric Red Fluorescent Protein that Tolerate Peptide Insertion and Testing of Corresponding Circular Permutations. Photochem Photobiol.
5 Shimozono S., Miyawaki A. (2008). Engineering FRET constructs using CFP and YFP. Methods Cell Biol.
6 Kolossov V.L., Spring B.Q., Sokolowski A., Conour J.E., Clegg R.M., Kenis P.J., Gaskins H.R. (2008). Engineering Redox-Sensitive Linkers for Genetically Encoded FRET-Based Biosensors. Exp Biol Med (Maywood).
7 Weissleder R., Ntziachristos V. (2003). Shedding light onto live molecular targets. Nat Med.
8 Lembert N., Idahl L.A. (1995). Regulatory effects of ATP and luciferin on firefly luciferase activity. Biochem J.
9 Matthews J.C., Hori K., Cormier M.J. (1977). Purification and properties of Renilla reniformis luciferase. Biochemistry.
10 Huang Q., Acha V., Yow R., Schneider E., Sardar D.K., Hornsby P.J. (2007). Bioluminescence measurements in mice using a skin window. J Biomed Opt.
11 Shah K., Tang Y., Breakefield X., Weissleder R. (2003). Real-time imaging of TRAIL-induced apoptosis of glioma tumors in vivo. Oncogene.
12 Tannous B.A., Kim D.E., Fernandez J.L., Weissleder R., Breakefield X.O. (2005). Codon-optimized Gaussia luciferase cDNA for mammalian gene expression in culture and in vivo. Mol Ther.
13 Verhaegen M., Christopoulos T.K. (2002). Recombinant Gaussia luciferase. Overexpression, purification, and analytical application of a bioluminescent reporter for DNA hybridization. Anal. Chem.
14 Wurdinger T., Badr C., Pike L., de Kleine R., Weissleder R., Breakefield X.O., Tannous B.A. (2008). A secreted luciferase for ex vivo monitoring of in vivo processes. Nat Methods.
15. Saeki, Y., X.O. Breakefield, and E.A. Chiocca, eds. Improved HSV-1 amplicon packaging system using ICP27-deleted oversized HSV-1 BAC DNA. Viral Vectors for Gene Therapy, Mathods and Protocols, ed. A. Curtis. 2003, Mashida Humana: Totowa, NJ. 51-60.
16 Aubert M., O'Toole J., Blaho J.A. (1999). Induction and prevention of apoptosis in human HEp-2 cells by herpes simplex virus type 1. J Virol.
17 Shaner N.C., Campbell R.E., Steinbach P.A., Giepmans B.N., Palmer A.E., Tsien R.Y. (2004). Improved monomeric red, orange and yellow fluorescent proteins derived from Discosoma sp. red fluorescent protein. Nat Biotechnol.
18 Badr C.E., Hewett J.W., Breakefield X.O., Tannous B.A. (2007). A highly sensitive assay for monitoring the secretory pathway and ER stress. PLoS ONE.
19 Colin M., Moritz S., Schneider H., Capeau J., Coutelle C., Brahimi-Horn M.C. (2000). Haemoglobin interferes with the ex vivo luciferase luminescence assay: consequence for detection of luciferase reporter gene expression in vivo. Gene Ther.